# ^64^Cu-Diethylenetriamine pentaacetic acid-NH-CO-CH_2_-S-CH_2_-Phe-Pro-Arg-CH_2_-prothrombin

Chemical name: | ^64^Cu-Diethylenetriamine pentaacetic acid-NH-CO-CH_2_-S-CH_2_-Phe-Pro-Arg-CH_2_-prothrombin
Abbreviated name: | ^64^Cu-DTPA-ProT
Synonym: | ^64^Cu-ProT
Agent Category: | Proteins
Target: | Staphylocoagulase
Target Category: | Bacterial enzyme
Method of detection: | Possitron emission tomography (PET)
Source of signal / contrast: | ^64^Cu (Copper-64)
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Staphylococcus%20aureus%20endocarditis%20and%20%20imaging)]

^64^Cu-Labeled diethylenetriamine pentaacetic acid (DTPA)-NH-CO-CH_2_-S-CH_2_-Phe-Pro-Arg-CH_2_-prothrombin, abbreviated as ^64^Cu-DTPA-ProT, is a probe synthesized by Panizzi et al. for detecting Staphylococcus aureus (S. aureus) endocarditis by targeting staphylocoagulase (1).

Infective endocarditis is a life-threatening condition that is commonly caused by S. aureus, and the hallmark of S. aureus endocarditis is the development of vegetations on heart valves (2). After entering into the bloodstream, S. aureus proliferates quickly, colonizes on either damaged or normal heart valves, and leads to a rapid progressive endocarditis with destruction of the heart valves (3-5). In this pathological process, adherence of S. aureus to heart valves is the key to initiate the vegetation formation, and SC is one of the most important stimulators of the initiation. SC is an extracellular protein secreted by coagulase-positive S. aureus, and it can bind prothrombin with a high affinity (K_d_ = ~17–72 pM) in a 1:1 stoichiometry (6-8). This binding forms an active SC-prothrombin complex, which induces plasma coagulation via specific cleavage of fibrinogen to fibrin (7, 9). The N-terminal D1 and D2 regions of SC are involved in the binding with prothrombin and its activation, and the C-terminal repeat region, comprising 27-amino-acid tandem repeats, is associated with the adherence of SC to fibrinogen (10, 11).

Panizzi et al. synthesized an engineered analog of human prothrombin in which the active site was modified by a thrombin inhibitor that possesses a protected thiol group (1, 6). Thus, the prothrombin analog could react with DTPA for ^64^Cu-labeling (^64^Cu-DTPA-ProT). The rationale underlying this design is the SC-dependent prothrombin recruitment, which simultaneously tethers the active SC-prothrombin analog complex into the fibrin(ogen)-rich S. aureus vegetations. Imaging studies by Panizzi et al. showed that the two probes could bind SC and intercalate into growing bacterial vegetations on the heart valves, with the potential to detect S. aureus endocarditis and monitor antibiotic therapy via noninvasive optical imaging and positron emission tomography (PET) (1).

This chapter summarizes the data obtained with ^64^Cu-DTPA-ProT, and another chapter summarizes the data obtained with the fluoroescent probe, AF680-ProT.

### Related Resource Links:

The nucleotide (http://www.ncbi.nlm.nih.gov/nuccore/?term=staphylocoagulase) and protein (http://www.ncbi.nlm.nih.gov/protein?term=staphylocoagulase) sequences of staphylocoagulase in GenBank

The structure of staphylocoagulase (http://www.ncbi.nlm.nih.gov/structure?term=staphylocoagulase)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/21857652)]

Panizzi et al. described the synthesis of ^64^Cu-DTPA-ProT in detail (1, 6). Prothrombin was purified from human plasma (absorption coefficient, 1.47 (mg/ml)−^1^cm−^1^; molecular weight, 71.6 kDa). Met-SC-(1–325)-His_6_ fragment was expressed in E. coli strain BL21(DE3) plysS and purified from the soluble fraction after centrifugation. An active site was first induced through the binding of Met-SC-(1–325)-His_6_ with prothrombin. This site was then inactivated via Ser^195^ and His^57^ alkylation with the thiol group-possessing thrombin inhibitor N^á^-[(acetylthio)acetyl]-D-Phe-Pro-Arg-CH_2_Cl (ATA-FPR-CH_2_Cl). The resulting Met-SC-(1–325)-His_6_·ATA-FPR-ProT complex was subsequently conjugated with maleimide-functionalized DTPA. Finally, the Met-SC-(1–325)-His_6_ was dissociated with NaSCN from the DTPA-conjugated complex, and the desired product, DTPA-ProT, was separated with gel filtration chromatography.

^64^Cu-DTPA-ProT was prepared by incubation of DTPA-ProT with ^64^CuCl_2_ in ammonium acetate buffer (0.4 M, pH 6.5) for 1 h at 40ºC. After cooling to room temperature, the reaction mixture was transferred to a centrifuge filter (50 kDa, Millipore), diluted with 100 μL phosphate-buffered saline (PBS), and centrifuged to remove unbound ^64^Cu. This dilution and concentration step was repeated four times until no activity was measured in the filtrate. ^64^Cu-DTPA-ProT (328.19 MBq (8.87 mCi)) collected on the filter was diluted in 200 μl PBS for experiments. The ^64^Cu incorporation by the DTPA-ProT was in a 89%–95% molar ratio (1). The specific activity of the final product was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/21857652)]

Panizzi et al. first determined the activity of the residual active prothrombin in the final product because the residual active prothrombin could trigger downstream activation of the clotting cascade in vivo (1). The results showed a residual activity of 0.2% for ^64^Cu-DTPA-ProT, indicating less potential to trigger clotting cascade when used in vivo.

Panizzi et al. then verified whether the recombinant N-terminal fragment SC (1–325) was able to activate mouse prothrombin. The investigators found that the SC (1–325)-prothrombin complex hydrolyzed the chromogenic substrate of H-D-Phe-Pip-Arg-pNA (S2238) at a rate that was equivalent to that of mouse thrombin (k_cat_ = 26 ± 1 s−^1^) (1, 6). The supernatants of various S. aureus strains were able to clot mouse plasma. These data indicate that the mouse is an appropriate model organism to study SC function and regulation in vivo.

To determine the molecular mechanism underlying prothrombin recruitment to vegetations, Panizzi et al. performed in vitro native gel binding experiments using either the N-terminal active fragment SC (1–325) or the full-length SC (1–660) (1, 6). After incubation of these SC forms with prothrombin and fibrinogen fragment D (FragD), SC (1–325) and prothrombin bound together but lacked the ability to interact with FragD. However, SC (1–660) formed an SC-prothrombin-FragD ternary complex, and multiple FragD subunits interacted with a single SC molecule. The SC recombinant fragment that contained only the pseudo-repeat and the first SC repeat could bind FragD with a K_d_ of 36 ± 8 nM. These results suggest that SC could interact with at least four fibrinogen or fibrin molecules per SC molecule to form a megaprotein complex, and this complex anchored the active SC-prothrombin complex to the growing vegetation.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/21857652)]

PET-CT imaging was performed at 12 h after injection of 34.04–59.94 MBq (0.92–1.62 mCi) ^64^Cu-DTPA-ProT in 12 mice with endocarditis induced by the genetically engineered S. aureus strain Xen8.1, which stably expresses luciferase at sites of infection (1).

PET-CT showed a robust localization of ^64^Cu-DTPA-ProT signal in the vegetations, consistent with ex vivo autoradiography (1). In mice without bacterial injection, no accumulation of ^64^Cu-DTPA-ProT was detected at the site of endothelial trauma. Bioluminescence signal from Xen8.1 was correlated with the ^64^Cu-DTPA-ProT accumulation (R^2^ = 0.94; P < 0.01), suggesting that the in vivo PET signal reflects the bacterial burden. Comparison of PET-CT imaging obtained with ^64^Cu-DTPA-ProT and with ^18^F-FDG–labeled leukocytes (identifying inflammatory foci) showed a higher vegetation/blood ratio (n = 5 mice; P < 0.05) for ^64^Cu-DTPA-ProT. Endocarditis was confirmed with Gram staining of the aortic valve and in situ bioluminescence.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently avaliable.

## References

1 Panizzi P., et al. (2011). In vivo detection of Staphylococcus aureus endocarditis by targeting pathogen-specific prothrombin activation. Nat Med.
2 Chorianopoulos E., et al. (2009). The role of endothelial cell biology in endocarditis. Cell Tissue Res.
3 Friedrich R., et al. (2003). Staphylocoagulase is a prototype for the mechanism of cofactor-induced zymogen activation. Nature.
4 Panizzi P., et al. (2004). The staphylocoagulase family of zymogen activator and adhesion proteins. Cell Mol Life Sci.
5 Hacisalihoglu A., et al. (2007). Restricted active site docking by enzyme-bound substrate enforces the ordered cleavage of prothrombin by prothrombinase. J Biol Chem.
6 Panizzi P., et al. (2006). Novel fluorescent prothrombin analogs as probes of staphylocoagulase-prothrombin interactions. J Biol Chem.
7 Panizzi P., et al. (2006). Fibrinogen substrate recognition by staphylocoagulase.(pro)thrombin complexes. J Biol Chem.
8 Friedrich R., et al. (2006). Structural basis for reduced staphylocoagulase-mediated bovine prothrombin activation. J Biol Chem.
9 Munnix I.C., et al. (2007). Segregation of platelet aggregatory and procoagulant microdomains in thrombus formation: regulation by transient integrin activation. Arterioscler Thromb Vasc Biol.
10 Watanabe S., et al. (2005). Structural comparison of ten serotypes of staphylocoagulases in Staphylococcus aureus. J Bacteriol.
11 Hirose M., et al. (2010). Identification of staphylocoagulase genotypes I-X and discrimination of type IV and V subtypes by multiplex PCR assay for clinical isolates of Staphylococcus aureus. Jpn J Infect Dis.